# Radioiodinated anti–TAG-72 non-covalently linked CC49 divalent single-chain Fv antibody

Chemical name: | Radioiodinated anti–TAG-72 non-covalently linked CC49 divalent single-chain Fv antibody
Abbreviated name: | ^125^I/^131^I-CC49 (scFv)_2_ Ab
Synonym: | ^125^I/^131^I-CC49 Ab, ^125^I/^131^I-CC49 divalent single-chain Fv recombinant antibody, ^125^I/^131^I-CC49 non-covalent (scFv)_2_ Ab, ^125^I/^131^I-dimeric single-chain Fv antibody construct
Agent Category: | Non-covalently linked CC49 divalent single-chain Fv antibody construct ((scFv)_2_ Ab)
Target: | (Sialyl-Tn (STn)) TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission tomography (SPECT), planar gamma imaging
Source of signal/ contrast: | ^125^I/^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))]

Radioiodinated anti–TAG-72 non-covalently linked CC49 divalent single-chain Fv antibody (^125^I/^131^I-CC49 (scFv)_2_ Ab), which is formed by the conjugation of ^125^I/^131^I with a bioengineered recombinant anti–tumor-associated glycoprotein 72 (TAG-72) antibody construct, has been developed for gamma imaging of cancers that express TAG-72 (1-4). ^125^I has a physical half-life (t_½_) of 60 days with a gamma energy that is not ideal for in vivo imaging. ^131^I has a physical half-life (t_½_) of 8.02 days with a gamma energy that is high but acceptable for in vivo imaging.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^6^ Da) with mucin-like characteristics (5-8). It is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (9). The murine monoclonal antibody B72.3 (MAb B72.3) against TAG-72 mucin was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (10). With the use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-72 MAbs with higher affinity constants (K_a_) have been produced and characterized (5, 6, 10, 11). CC49 MAb appears to react with a unique disaccharide sialyl-Tn (STn) epitope on TAG-72 (2, 4).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (12). Radiolabeled B72.3 and CC49 exhibit excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (13, 14). Because of their relatively large size, intact radiolabeled MAbs tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (11, 15-17). One approach to minimize these problems is reducing intact antibodies to antibody fragments such as F(ab’)_2_ and Fab’ (18). Another approach is the development of genetic engineering methods to obtain single-chain Fv constructs (scFv) and multivalent scFv constructs (11, 19, 20). These scFv constructs contain the variable regions of the light chain (V_L_) and heavy chain (V_H_) connected by a flexible linker. Colcher et al. (21) constructed the monomeric CC49 scFv Ab (~27 kDa), which selectively recognizes a unique STn epitope of TAG-72. The radioiodinated CC49 scFv appeared to clear rapidly from the blood with good tumor penetration (1, 20). To further improve the imaging kinetics by use of multivalency as a means of increasing the functional affinity, a non-covalently linked dimeric scFv was isolated on the basis of the spontaneous formation of the dimer from the monomeric CC49 scFv (1, 2, 4). This dimeric scFv was designated (scFv)_2_ to distinguish it from the covalently-linked dimer sc(Fv)_2_, in which two repeating chains of V_L_ and V_H_ are covalently linked in tandem (4). The radioiodinated CC49 (scFv)_2_ showed good stability and improved in vivo pharmacokinetics compared with the intact CC49 IgG.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))+AND+synthesis)]

Beresford et al. (4) and Pavlinkova et al. (1, 3) reported the construction and radiolabeling of the^125^I/^131^I-CC49 (scFv)_2_ Ab. The covalent CC49 scFv (V_L_-linker-V_H_) was derived from the murine MAb CC49 and constructed with the 205C linker with 25 amino acids (LSADDAKKDAAKKDDAKKDDAKKDL) (22). The sequence was confirmed by deoxyribonucleic acid sequencing. The fragment was cloned into the pRW83 vector, which contained a chloramphenicol resistance gene for recombination selection, the pen P gene with a penP promoter and terminator, and a pe1B signal peptide that directed the recombinant protein to the periplasmic space to produce the biologically active protein (4). The expression plasmid was transformed into Escherichia coli strain AG1. When expressed, this construct spontaneously formed the monomeric CC49 scFv and dimeric CC49 (scFv)_2_. These soluble proteins were purified by ion-exchange chromatography, and CC49 (scFv)_2_ was separated from CC49 scFv by gel filtration chromatography on a Superdex 75 column. The preparation was shown to be >90% pure by sodium dodecylsulfate–polyacrylamide gel electrophoresis (SDS-PAGE), and the protein migrated to its theoretical molecular weight of 60,000 (3).

Radioiodination of CC49 (scFv)_2_ Ab was performed with the use of 1,3,4,6-tetrachloro-3α,6α-diphenylglycoluril (IodoGen) as the oxidizing agent (1, 3, 4). Briefly, 20–100 μg of CC49 (scFv)_2_ Ab in 0.1 M sodium phosphate buffer (pH 7.2) was added to a glass tube coated with 20 μg IodoGen. Approximately 0.014–0.027 MBq (0.5–1.0 mCi) ^131^I-labeled sodium iodide ([^131^I]NaI) or ^125^I-NaI was added and the mixture was incubated for 3 min. Size-exclusion chromatography on a Sephadex G-25 column was performed immediately to purify the radiolabeled antibody. The labeling efficiency was ~90% by high-performance liquid chromatography (HPLC) (4). The specific activity of ^125^I/^131^I-CC49 (scFv)_2_ Ab was ~111–333 MBq/mg (3–9 mCi/mg) or 6.66–19.98 MBq/nmol (0.18–0.54 mCi/nmol) on the basis of the molecular mass of 60 kDa. The SDS-PAGE analysis showed that the non-covalently linked ^131^I-CC49 (scFv)_2_ was dissociated by the SDS and appeared only as its 30-kDa form. The radiochemical purity was >90% (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))AND+in+vitro)]

The immunoreactivity of radioiodinated CC49 (scFv)_2_ Ab was assessed by solid-phase radioimmunoassay (RIA), with bovine submaxillary gland mucin (BSM) as the protein antigen attached to a solid-phase matrix (1, 2, 4). The specific binding for ^125^I/^131^I-CC49 (scFv)_2_ Ab was 88–94%. The binding kinetics of ^125^I/^131^I-CC49 (scFv)_2_ Ab was assessed by the real-time kinetic analysis with use of a surface plasmon resonance detector (4). The study reported the association constant (K_a_) of unlabeled CC49 (scFv)_2_ to be 4.46 × 10^7^ M−^1^ (1-4). In comparison, the K_a_ for the intact CC49 MAb was 1.14 × 10^8^ M−^1^. The relative affinity constant of^125^I/^131^I-CC49 (scFv)_2_ calculated from the Scatchard plot of the data obtained from the competition enzyme-linked immunosorbent assay was 1.70 × 10^9^ M−^1^ (1).

In vitro stability studies of ^125^I/^131^I-CC49 (scFv)_2_ Ab showed that it was stable for at least 35 days when stored at 4ºC (1, 4). No significant protein degradation or radioactive iodine release was determined by HPLC and radioimmunoassay. Only ~2–3% loss in immunoreactivity was exhibited (1). Unlabeled (scFv)_2_ was stable at −70ºC for >10 months without loss of immunoreactivity (1). When ^125^I/^131^I-CC49 (scFv)_2_ Ab was incubated in murine serum or 1% bovine serum albumin and incubated at 37ºC for up to 4 days, HPLC analysis showed that radioiodinated CC49 (scFv)_2_ maintained its full integrity (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))+AND+rodentia)]

Biodistribution studies of ^131^I-CC49 (scFv)_2_ Ab were performed in nude mice bearing s.c. LS-174T human colon carcinomas (2, 4). Dual-label biodistribution studies were conducted with simultaneous i.v. administration of 0.0925 MBq (2.5 μCi) ^131^I-CC49 (scFv)_2_ Ab and 0.185 MBq (5 μCi) ^125^I-covalently-linked CC49 sc(Fv)_2_ Ab. The groups of mice (n = 5−6 per group) were euthanized at various time points. Similar separate experiments were performed for intact, radioiodinated CC49 IgG. The average tumor radioactivity levels of ^131^I-CC49 (scFv)_2_ Ab in percent injected dose per gram (% ID/g) were 5.94 (0.5 h), 6.37 (1 h), 6.91 (4 h), 6.45 (6 h), 5.52 (9 h), 4.48 (16 h), 4.29 (24 h), 2.56 (48 h), 1.92 (72 h), and 1.20 (120 h) with standard errors (SEM) <20% ID/g. There were also high radioactivity levels in the kidneys, spleen, blood, lungs, and liver at 0.5 h. By 24 h, these major organ radioactivity levels (% ID/g) decreased to 0.10 (blood), 0.42 (kidneys), 0.45 (spleen), 0.30 (liver), 0.09 (lungs), and 0.04 (heart). The rapid clearance from the major organs and the blood was favorable when compared with intact CC49 IgG. The tumor/blood ratios of ^131^I-CC49 (scFv)_2_ Ab were 4.19 (6 h), 44.05 (24 h), 41.09 (48 h), 29.75 (72 h), and 26.90 (120 h). In comparison, the tumor/blood ratios of radioiodinated CC49 IgG were 1.34 (6 h), 4.19 (24 h), 8.53 (48 h), and 51.52 (120 h). The radiolocalization indexes (ratios of % ID/g in tumor to % ID/g in normal tissue) at 24 h for ^131^I-CC49 (scFv)_2_ Ab were 42.9 (tumor/blood), 14.3 (tumor/liver), 9.5 (tumor/spleen), 10.2 (tumor/kidneys), and 47.7 (tumor/lungs). The 24-h radiolocalization indexes for radiolabeled CC49 IgG were 3.4 (tumor/blood), 6.1 (tumor/liver), 9.1 (tumor/spleen), 17.3 (tumor/kidneys), and 7.2 (tumor/lungs). The ^125^I-covalently linked CC49 sc(Fv)_2_ Ab had similar tumor localization, but there were differences in the degree of clearance from other normal tissues.

Pharmacokinetic studies of ^131^I-CC49 (scFv)_2_ Ab were conducted in mice bearing s.c. LS-147 tumors with a dose of 0.37 MBq (10 μCi) (4). ^131^I-CC49 (scFv)_2_ Ab showed rapid blood clearance with >50% cleared from the blood pool in <40 min. ^131^I-CC49 (scFv)_2_ Ab appeared to be eliminated by the kidneys and not retained by the extravascular space. Whole-body retention studies with a dose of 0.056 MBq (1.5 μCi) in mice bearing the tumors (n = 3) also showed rapid blood clearance. The ^125^I-CC49 sc(Fv)_2_ Ab showed similar pharmacokinetics and blood clearance. In another study, Pavlinkova et al. (3) reported that ^131^I-CC49 (scFv)_2_ had faster blood and whole-body clearances than those of CC49 IgG and CC49 (Fab’)_2_.

Pavlinkova et al. (1, 3) also compared CC49 (scFv)_2_ with CC49 F(ab’)_2_ in mice (n = 6) bearing s.c. LS-174T carcinomas. Dual-label biodistribution studies were conducted with simultaneous i.v. administration of 0.0925 MBq (2.5 μCi) ^131^I-CC49 (Fab’)_2_ and 0.185 MBq (5 μCi) ^125^I-CC49 (scFv)_2_. In this study, the tumor radioactivity levels of ^125^I-CC49 (scFv)_2_ were higher than those reported by Beresford et al. (4). The radiolocalization indexes at 24 h for ^125^I-CC49 (scFv)_2_ were 80.3 (tumor/blood), 25.5 (tumor/liver), 31.2 (tumor/spleen), 21.6 (tumor/kidneys), and 80.3 (tumor/lungs). In comparison, the radiolocalization indexes for ^131^I-CC49 (Fab’)_2_ were 16.7 (tumor/blood), 12.5 (tumor/liver), 20.5 (tumor/spleen), 13.4 (tumor/kidneys), and 29.5 (tumor/lungs).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))++AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))++AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((single-chain+antibody+construct+of+MAb+CC49)+OR+(sc(Fv)2+CC49))+AND+human)]

No publication is currently available.

## References

1 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.
2 Colcher D., Pavlinkova G., Beresford G., Booth B.J., Batra S.K. (1999). Single-chain antibodies in pancreatic cancer. Ann N Y Acad Sci.
3 Pavlinkova G., Booth B.J., Batra S.K., Colcher D. (1999). Radioimmunotherapy of human colon cancer xenografts using a dimeric single-chain Fv antibody construct. Clin Cancer Res.
4 Beresford G.W., Pavlinkova G., Booth B.J., Batra S.K., Colcher D. (1999). Binding characteristics and tumor targeting of a covalently linked divalent CC49 single-chain antibody. Int J Cancer.
5 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
6 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
7 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
8 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
9 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
10 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
11 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
12 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
13 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
14 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
15 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
16 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
17 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
18 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55Suppl23 5777s 5785s 7493346
19 Bird R.E., Hardman K.D., Jacobson J.W., Johnson S., Kaufman B.M., Lee S.M., Lee T., Pope S.H., Riordan G.S., Whitlow M. (1988). Single-chain antigen-binding proteins. Science.
20 Colcher D., Bird R., Roselli M., Hardman K.D., Johnson S., Pope S., Dodd S.W., Pantoliano M.W., Milenic D.E., Schlom J. (1990). In vivo tumor targeting of a recombinant single-chain antigen-binding protein. J Natl Cancer Inst.
21 Colcher D., Goel A., Pavlinkova G., Beresford G., Booth B., Batra S.K. (1999). Effects of genetic engineering on the pharmacokinetics of antibodies. Q J Nucl Med.
22 Pavlinkova G., Beresford G., Booth B.J., Batra S.K., Colcher D. (1999). Charge-modified single chain antibody constructs of monoclonal antibody CC49: generation, characterization, pharmacokinetics, and biodistribution analysis. Nucl Med Biol.